# Mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly conjugated to Cy5.5

Chemical name: | Mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly conjugated to Cy5.5 | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Abbreviated name: | c-MBP-GGG-Cy5.5 | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Synonym: | | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Agent Category: | Ligand | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Target: | Mesenchymal-epithelial transition factor receptor (c-Met); hepatocyte growth factor receptor (HGFR) | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Target Category: | Receptor | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Method of detection: | Near-infrared fluorescence (NIR) imaging | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Source of signal / contrast: | Cy5.5 | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Activation: | No | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-Gly-Gly-Gly-Ser-Cys-Cy5.5
Studies: | - In vitro; - Rodents | Structure of cBMP-GGG-Cy5.5

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5)]

The hepatocyte growth factor (HGF) is the only known ligand of the mesenchymal-epithelial transition factor (c-Met) (also known as the HGF receptor) that has an important function, including cell development, proliferation, scattering, migration, and angiogenesis, all of which are necessary for the survival and repair of tissues (1). c-Met is known to mediate its activity through an intracellular tyrosine kinase (TK) that activates different signal transduction pathways, leading to initiation of the various cell processes (2). Also, deregulation of c-Met activity due to paracrine/autocrine activation, overexpression, or a mutation promotes the development of a neoplastic cell phenotype (2). Overexpression of c-Met and HGF has been associated with a poor prognosis and survival of the patient (3), suggesting that the c-Met receptor may be a suitable target for the detection of cancers at an early stage, which could help in the development of an appropriate treatment regimen to improve patient prognosis (4). c-Met is the target of several drugs under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=HGFR) approved by the United States Food and Drug Administration. Investigators recently generated a monoclonal antibody (mAb) that inhibits the HGF–c-Met interaction and identified the active mAb epitope peptide as KSLSRHDHIHHH, which was designated as the c-Met binding peptide (cMBP) (5). The cMBP and its derivatives (containing either a tri-amino acid linker, Gly-Gly-Gly (GGG), or an aliphatic carbon linker, 8-aminooctanoic acid (AOC)) were labeled with ^125^I to generate ^125^I-cMBP, 1^25^I-cMBP-GGG, and ^125^I-cMBP-AOC, and these agents were used to detect c-Met TK-positive tumor xenografts in mice (6). From this study the investigators concluded that although ^125^I-cMBP-GGG was a suitable imaging agent for the c-Met–positive tumors, the imaging signal could probably be improved by either changing the linker or by using a different nuclide or source of signal (such as an optical imaging agent).

In an attempt to generate a c-Met–positive tumor imaging agent superior to the ^125^I- cMBP-GGG, investigators conjugated a near-infrared (NIR) fluorescent dye, cyanine 5.5 (Cy5.5), to cMBP-GGG and cMBP-AOC to obtain cMBP-GGG-Cy5.5 and cMBP-AOC-Cy5.5 (4). The Cy5.5-conjugated cMBP derivatives were then evaluated for the NIR imaging of c-Met–positive xenograft tumors in a mouse model. This chapter describes the characterization of only cMBP-GGG-Cy5.5. The other c-Met imaging agents (^125^I-cMBP, 1^25^I-cMBP-GGG, ^125^I-cMBP-AOC, and cMBP-AOC-Cy5.5) are described in separate MICAD chapters (7-10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of cMBP and cMBP-GGG-Cy5.5 has been described previously (4). Briefly, the cMBP-GGG peptide was synthesized using Fmoc chemistry, and it was mixed with Cy5.5-maleimide for 6 h in the dark at room temperature. The GGG and Cy5.5 were bound to the C-terminus of the cBMP and the GGG, respectively. The crude cMBP-GGG-Cy5.5 product was purified with dialysis using a 2,000 molecular weight cut-off membrane. The typical yield of cMBP-GGG-Cy5.5 was reported to be >65%. The molecular mass of the purified cMBP-GGG-Cy5.5 was determined with matrix-assisted laser desorption/ionization time-of-flight mass spectroscopy. The final product was analyzed with reverse-phase high-performance liquid chromatography (RP-HPLC). The purity of cMBP-GGG-Cy5.5 was reported to be >90% as determined with RP-HPLC. The absorption and fluorescence characteristics of cMBP-GGG-Cy5.5 were determined in water with the use of an ultraviolet-visible spectrophotometer, and the spectra of the Cy5.5-labeled peptide were reported to be similar to free Cy5.5. Stability of the Cy5.5-labeled peptide was not reported.

For some in vitro studies, ^125^I-labeled cMBP was also used, and this radiolabeled compound was prepared as described before (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

A soluble human c-Met/Fc chimeric protein was purchased from a commercial source and used for an in vitro ^125^I-cMBP displacement binding assay using cMBP and cMBP-GGG-Cy5.5, respectively (4). The 50% inhibitory concentration values of cMBP and cMBP-GGG-Cy5.5 were determined to be 1.5 μM and 318 nM, respectively. In another study, human U87MG glioma cells were exposed to cMBP-GGG-Cy5.5in presence or absence of non-fluorescent cBMP (86 nmol) and cell fluorescence was acquired 1 h later (4). Only cells exposed to cMBP-GGG-Cy5.5 were reported to show fluorescence that was inhibited by the presence of excess unlabeled cMBP. Confocal microscopy revealed that cMBP-GGG-Cy5.5 bound only to the cell surface and was not internalized by the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+rodentia)]

NIR fluorescence imaging was performed on athymic mice (the number of animals used per time point was not reported) bearing U87MG cell xenograft tumors at predetermined time points for up to 24 h after injection of cMBP-GGG-Cy5.5 through the tail vein (4). For comparison, another group of animals was injected with cMBP-AOC-Cy5.5. Fluorescence imaging of the two groups of animals showed that the signals from both conjugates were visible primarily in the tumor, kidney, and the bladder regions of the animals. The tumor/muscle (T/M) ratios for the two conjugates were generated for the different time points after imaging. With cMBP-GGG-Cy5.5, the ratio was observed to increase from ~3 at 10 min to ~13 at 17 h, and it remained stable thereafter up to 24 h. A similar trend was noticed with cMBP-AOC-Cy5.5, but the fluorescence with this conjugate was consistently approximately three-fold higher than that obtained with cMBP-GGG-Cy5.5. No blocking studies were reported for cMBP-GGG-Cy5.5.

From these studies the investigators concluded that although cMBP-GGG-Cy5.5 was a suitable imaging agent for c-Met–expressing tumors, it was not superior to cMBP-AOC-Cy5.5 for imaging purposes (because cMBP-AOC-Cy5.5 had an ~3-fold higher fluorescence than cMBP-GGG-Cy5.5 in the tumors).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Naran S., Zhang X., Hughes S.J. (2009). Inhibition of HGF/MET as therapy for malignancy. Expert Opin Ther Targets.
2 Abounader R., Laterra J. (2005). Scatter factor/hepatocyte growth factor in brain tumor growth and angiogenesis. Neuro Oncol.
3 Birchmeier C., Birchmeier W., Gherardi E., Vande Woude G.F. (2003). Met, metastasis, motility and more. Nat Rev Mol Cell Biol.
4 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Jeong H.J., Kim D.W., Lim S.T., Sohn M.H. (2009). In vivo imaging of mesenchymal-epithelial transition factor (c-Met) expression using an optical imaging system. Bioconjug Chem.
5 Kim K., Hur Y., Ryu E.K., Rhim J.H., Choi C.Y., Baek C.M., Lee J.H., Chung J. (2007). A neutralizable epitope is induced on HGF upon its interaction with its receptor cMet. Biochem Biophys Res Commun.
6 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Kim D.W., Jeong H.J., Lim S.T., Sohn M.H., Kim K., Chung J. (2009). Characterization, biodistribution and small-animal SPECT of I-125-labeled c-Met binding peptide in mice bearing c-Met receptor tyrosine kinase-positive tumor xenografts. Nucl Med Biol.
7 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide [125I-cMBP]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide with a Gly-Gly-Gly linker. [125I-cMBP-GGG]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide an 8-aminooctanoic acid linker. [125I-cMBP-AOC]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., Mesenchymal-epithelial transition factor binding peptide with an 8-aminooctanoic acid linker conjugated to Cy5.5. [cMBP-AOC-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.